# ^124^I-Annexin V

Chemical name: | ^124^I-Annexin V
Abbreviated name: | ^124^I-Anx5
Synonym: | ^124^I-MBP-Annexin V, ^124^I-Annexin A5, ^124^I-Anx A5, [^124^I]m-IBA-Anx5, [^124^I]4IB-Anx5, [^124^I]SIB-Anx5.
Agent Category: | Protein
Target: | Phosphatidylserine (PS)
Target Category: | Receptor binding
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^124^I
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=430966), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nucleotide&val=4809273) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=308) for more information about Annexin V

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28124I-Annexin%20V%29%20OR%20%28radioiodinated%20annexin%20v%29)]

^124^I-Annexin V (^124^I-Anx5) is a radioiodinated protein molecule developed for positron emission tomography (PET) imaging of programmed cell death (apoptosis) (1, 2). ^124^I is a positron emitter with a relatively long physical t_½_ of 4.2 d.

Apoptosis is an essential biological process that maintains homeostasis of tissues and organs in concert with proliferation, growth, and differentiation (3, 4). Cell death can occur by the process of necrosis or by the process of apoptosis. Apoptosis is a highly regulated, genetically-controlled, noninflammatory, and ATP-requiring process (5). The apoptotic process can be triggered either by a decrease in factors required to maintain the cell in good health or by an increase in factors that causes cells to die (6). The two known mechanisms of apoptosis are the death receptor (extrinsic) and the mitochondrial (intrinsic) pathways (7). Annexin V (Anx5) is one of the numerous members of the calcium and phospholipids binding superfamily of annexin proteins. The mature Anx5 molecule consists of 319 amino acids with a total molecular weight of 35.8 kDa. Most of the biological functions of annexin are based on its high affinity for negatively charged phospholipids in the presence of physiological concentrations of calcium. Anx5 binds to membrane-bound phophatidylserine (PS) which is normally restricted to the inner leaflet of the plasma membrane lipid bilayer (6). PS is exposed on the surfaces of cells as they undergo apoptosis. This change in the membrane can be detected by the binding of Anx5 to the external PS (2, 7, 8). It is also possible that Anx5 may bind to PS exposed on the cell surface in pathological conditions associated with necrosis and vascular damage.

Anx5 has been labeled with various radionuclides for single photon emission computed tomography imaging and PET imaging of apoptosis (7, 9). The long physical t_½_ of ^124^I allows for the possibilities for monitoring and quantification of long-term biological processes involving Anx5 (7). The detection and quantification of cell death in vivo have potential clinical value for diagnosis and assessment of therapeutic efficacy in transplanted organ rejections, autoimmune deficiency syndrome, septic shock, cardiovascular diseases, neurodegenerative disorders, and cancer. Anx5 was originally obtained from human tissue. Currently, recombinant human Anx5 (rh Anx5) can be produced in high yields with excellent purity by bioengineering techniques. Direct radioiodination of Anx5 proteins has been performed by means of electrophilic aromatic substitution of the molecule’s tyrosine residues (10). Alternatively, Anx5 has also been radioiodinated indirectly by use of prelabeled reagents (1). Because of their structural similarity to thyroxine, the directly iodinated proteins are more likely subject to in vivo deiodination than the indirectly iodinated proteins (11).

## Synthesis

PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28124I-Annexin%20V%29%20OR%20%28radioiodinated%20annexin%20v%29%20AND%20synthesis)]

Glaser et al. (12) compared two ^124^I radioiodination methods to label annexin V (wild-type and polyhistidine-labeled recombinant Anx5). Anx5 was radioiodinated directly by the chloramine-T (CAT) method and indirectly by N-succinimidyl-3-[^124^I]iodobenzoate ([^124^I]m-SIB). [^124^I]Iodide was produced by the ^124^Te(p,n)^124^I reaction using 12.5 MeV proton irradiation. The specific activity of sodium [^124^I]iodide obtained was 27.6 GBq/μmol (0.75 Ci/μmol). In the CAT method, sodium [^124^I]iodide was mixed with 1 M hydrochloric acid and sodium phosphate buffer. Anx5 (2.78 х 10−^10^ mol) and CAT (5 μg) in sodium phosphate buffer were added and incubated for 5 min at pH 6.5 at room temperature. A solution of m-tyrosine solution was then added for another 5 min of incubation. Labeling efficiency was nearly 80%. After gel filtration purification, the radiochemical yield of ^124^I-Anx5 was 22.3 ± 2.6% (n = 3) with a radiochemical purity of 97.7 ± 1.0%. The specific activity was reported to be 14.5 GBq/μmol (0.39 Ci/μmol). In the indirect method, N-acylation of Anx5 lysine amino acid residues was used to produce a [^124^I]m-iodobenzoate conjugation product. [^124^I]m-SIB was first prepared from N-succinimidyl-3-(tri-methylstannyl) benzoate and then radiolabeled by IodoGen with a radiochemical yield of 39.3 ± 8.4% (n = 3) and a radiochemical purity of 98.7 ± 0.4% (13). Anx5 was incubated with [^124^I]m-SIB in borate buffer for 1 h at pH 8.5 at 0 ºC (14). [^124^I]m-IBA-Anx5 was then purified by fast protein liquid chromatography or gel filtration with a radiochemical yield of 14% or 25%, respectively. The radiochemical purity was 96.7 ± 2.1% (n = 3), and the specific radioactivity was 1.61 GBq/μmol (0.044 Ci/μmol).

Keen et al. (15) and Dekker et al. (1) reported the direct radioiodination of placental Anx5 and recombinant maltose-binding protein/Anx5 chimera (MBP-Anx5) by 1,3,4,6-tetrachloro-3α,6α-diphenylglycouril (IodoGen) coated on microfuge tubes. ^124^I was produced by the ^126^Te(p,3n)^124^I reaction with a radionuclide purity of 95-98%. Briefly, Anx5 and [^124^I]NaI in binding buffer were dispensed into the IodoGen-coated microfuge tubes and incubated at room temperature for 20 min. The final product of ^124^I-Anx5 was purified by gel filtration. The overall labeling efficiency was 20-70%. The authors suggested that the wide variations in efficiency were due to the presence of iodate in the total trapped ^124^I activity. Dekker et al. (16) also conducted indirect iodination of Anx5 by using [^124^I]N-hydroxysuccinimidyl-4-iodobenzoate. This prelabeled reagent was prepared by iododestannylation of N-hydroxysuccinimidyl-4-(tributylstannyl)benzoate. [^124^I]N-hydroxysuccinimidyl-4-iodobenzoate was produced from radiolabeling N-hydroxysuccinimidyl-4-(tributylstannyl)benzoate with ^124^I in the presence of N-chlorosuccinimide and 5% acetic acid. Finally, Anx5 in borate buffer (pH 8.5) was incubated with this ^124^I-labeled reagent on ice for 2 h or at room temperature for 15 min to produce the [^124^I]41B-Anx5. The radiochemical yield was 20-30% after gel filtration purification.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28124I-Annexin%20V%29%20OR%20%28radioiodinated%20annexin%20v%29%20AND%20in%20vitro)]

The in vitro storage stability of ^124^I-Anx5 (CAT labeling) and [^124^I]m-IBA-Anx5 ([^124^I]m-SIB labeling) was studied (12). Both preparations of <5 MBq (0.14 mCi) radioactivity appeared to be stable at 4 ºC for about 4 d without any noticeable deiodination. The in vitro biological activity of these two preparations was studied in human leukemia cells HL60. These cells were treated with the topoisomerase inhibitor camptothecin (CPT; 5 μM in dimethyl sulfoxide (DMSO)), to induce apoptosis. [^124^I]m-IBA-Anx5 showed 21% (P<0.05) higher binding with treated cells than with untreated cells. These bindings were decreased by 68% and 60% when pre-incubated with a 100-fold excess of unlabeled Anx5 for treated and untreated cells, respectively. ^124^I-Anx5 showed only 17% (P<0.05 in only one out of three studies) higher binding in treated cells because of possible reduced biological activity. When HL60 cells were heated at 50ºC for 1 h to force the PS exposure, [^124^I]m-IBA-Anx5 had a 56% increase in binding to heated cells (14). Lahorte et al. (7) suggested that the DMSO solvent used for dissolving CPT was capable of inducing apoptosis in control cells. These preparations were also studied in drug-induced apoptosis in tumors by using RIF-1 fibrosarcoma cells treated with 5-fluorouracil (5-FU). In these clonogenic survival studies, ^125^I was used instead of ^124^I. Both ^124^I-Anx5 and [^124^I]m-IBA-Anx5 showed higher binding in treated cells compared to untreated cells (17). There was also a large decrease in binding after pretreatment with unlabeled Anx5.

Dekker et al. (16) tested the in vitro biological activity of ^124^I-Anx5 (IodoGen) and [^124^I]41B-Anx5 ([^124^I]N-hydroxysuccinimidyl-4-iodobenzoate labeling) in CPT-treated Jurkat cells. [^124^I]4IB-Anx5 exhibited approximately four times greater binding to treated cells than that of untreated cells. Keen et al. (15) reported that ^124^I-Anx5 showed 7.5 times greater binding in treated cells. In another study, flow cytometry confirmed that the CPT-treated cells contained a large apoptotic population. Dekker et al. (1) also found significantly greater binding to treated Jurkat cells for [^124^I]-MBP-Anx5 (recombinant maltose-binding protein/annexin V chimera, IodoGen), there was an eight-fold increase in binding to treated cells compared to untreated cells (18).

Dekker et al. (16) used PS-enzyme-linked immunosorbent assay (ELISA) to study the in vitro activity of radioiodinated annexin V. Good linear correlations were found for both [^124^I]41B-Anx5and [^124^I]-Anx5 (IodoGen) with the gradient of [^124^I]4IB-Anx5 being steeper indicating that its PS-binding rate was faster. Dekker et al. (1) used ^125^I labeling to show that both radioiodinated (IodoGen) MBP-Anx5 and placental Anx5 bound to PS in the ELISA.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28124I-Annexin%20V%29%20OR%20%28radioiodinated%20annexin%20v%29%20AND%20rodentia)]

Collingridge et al. (17) used [^125^I]m-IBA-Anx5 (polyhistidine-labeled recombinant Anx5) for 2−120 min distribution studies in RIF-1−bearing mice. The tissue radioactivity uptake was rapid and the washout was slower, with the highest radioactivity levels in all tissues found at 2 min. The highest radioactivity was observed in kidneys and urine. For tumor uptake, the 60-min tumor/blood ratios of [^125^I]m-IBA-Anx5 radioactivity were 0.84 ± 0.16 (n = 3-10), 0.36 ± 0.05, and 0 for 5−FU−treated (165 mg/kg), untreated, and unlabeled Anx5 pretreatment, respectively. In comparison, the 60-min tumor/blood uptake ratio values for ^125^I-Anx5(CAT) were 0.99 ± 0.05, 0.94 ± 0.17, and 0.55 ± 0.03, respectively. PET imaging with [^124^I]m-IBA-Anx5 (370 kBq (10 μCi)) and ^124^I-Anx5 (1480 kBq (40 μCi)) at 30−60 min after injection showed high kidney and bladder radioactivity in 5−FU−treated mice. There was thyroid (unblocked) activity with the ^124^I-Anx5 mouse. The tumors were not visualized in either case.

Keen et al. (15) and Dekker et al. (16) studied the biodistribution of ^124^I-Anx5 (IodoGen) and [^124^I]4IB-Anx5 ([^124^I]N-hydroxysuccinimidyl-4-iodobenzoate labeling) in a mouse model of anti-Fas antibody−induced hepatic apoptosis. Each mouse received approximately 0.1 MBq (2.7 μCi) of the radiolabeled protein by i.v. injection and was euthanized 2 h after injection. The major organ radioactivity levels (percent injected dose/g (% ID/g); n = 4) for ^124^I-Anx5 in anti-Fas−treated mice were 57 ± 9 (liver), 40 ± 26 (urine), 11 ± 5.3 (stomach content), 6.7 ± 1.2 (blocked thyroid), 4.5 ± 0.2 (kidney), and 5.7 ± 1.0 (blood). The radioactivity of ^124^I-Anx5 was rapidly cleared from the blood with a t_½_<12 min. High-performance liquid chromatography (HPLC) of urine radioactivity at 2 h showed that it was all in the form of unbound ^124^I−_._ In the liver, at 2 h after administration 70% of the radioactivity was ^124^I-Anx5, 15% was a high molecular weight metabolite, and 12% was radioactive iodide at 2 h after administration. In PET imaging of the treated mouse, there was a very high liver radioactivity which was 17 times greater than that in the untreated mouse. There was a strong correlation between the apoptotic density (AD) in the liver determined by histology and the biodistribution/PET imaging data. For [^124^I]4IB-Anx5, the organ radioactivity levels (%ID/g) were 25 ± 7.7 (liver), 127 ± 118 (urine), 2.0 ± 2.8 (stomach content), 7.6 ± 2.3 (blocked thyroid), 20 ± 10 (kidney), and 4.1 ± 2.6 (blood) (16). There was a significantly higher hepatic accumulation of both preparations in treated mice with hepatic apoptosis than seen in untreated mice. The liver radioactivity levels in untreated mice were 2.1 ± 1.0% ID/g and 4.1 ± 3.0% ID/g for ^124^I-Anx5 (IodoGen) and [^124^I]4IB-Anx5, respectively. These uptake values correlated well with ex vivo histology studies of AD in the liver. PET imaging of the treated mice injected with [^124^I]4IB-Anx5 revealed high radioactivity in the liver. HPLC and PS−binding assays of liver samples from the imaging animals positively identified [^124^I]4IB-Anx5. HPLC analysis of kidney and urine samples indicated that the predominant form of radioactivity was a low molecular weight metabolite.

Dekker et al. (1) reported the biodistribution (0.1−1 MBq (2.7−27 μCi)) and PET imaging (2−4 MBq (54−108 μCi)) studies of ^124^I-MBP-Anx5 (maltose-binding protein/annexin V chimera; IodoGen) in anti-FAS−treated mice. In untreated mice, there was negligible uptake in all tissues except the thyroid (blocked), urine, and stomach content. Liver radioactivity (n = 4) of ^125^I-MBP-Anx5 was nine times greater in treated mice (20.4 ± 5.5% ID/g) than in untreated mice (2.3 ± 0.3% ID/g). This was confirmed by ^124^I-MBP-Anx5 PET imaging. Immunohistochemistry showed good correlation of AD and radioactivity distribution in the liver.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28124I-Annexin%20V%29%20OR%20%28radioiodinated%20annexin%20v%29%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No publication is currently available.

### Non-Human Primates

PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28124I-Annexin%20V%29%20OR%20%28radioiodinated%20annexin%20v%29%20AND%20non-human%20primates)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28124I-Annexin%20V%29%20OR%20%28radioiodinated%20annexin%20v%29%20AND%20human)]

No publication is currently available.

## References

1 Dekker B., Keen H., Lyons S., Disley L., Hastings D., Reader A., Ottewell P., Watson A., Zweit J. (2005). MBP-annexin V radiolabeled directly with iodine-124 can be used to image apoptosis in vivo using PET. Nucl Med Biol.
2 Blankenberg F.G. (2004). Recent advances in the imaging of programmed cell death. Curr Pharm Des.
3 Bohm I., Schild H. (2003). Apoptosis: the complex scenario for a silent cell death. Mol Imaging Biol.
4 Kerr J.F., Wyllie A.H., Currie A.R. (1972). Apoptosis: a basic biological phenomenon with wide-ranging implications in tissue kinetics. Br J Cancer.
5 Brauer M. (2003). In vivo monitoring of apoptosis. Prog Neuropsychopharmacol Biol Psychiatry.
6 Van de Wiele C., Vermeersch H., Loose D., Signore A., Mertens N., Dierckx R. (2004). Radiolabeled annexin-V for monitoring treatment response in oncology. Cancer Biother Radiopharm.
7 Lahorte C.M., Vanderheyden J.L., Steinmetz N., Van de Wiele C., Dierckx R.A., Slegers G. (2004). Apoptosis-detecting radioligands: current state of the art and future perspectives. Eur J Nucl Med Mol Imaging.
8 Narula J., Kietselaer B., Hofstra L. (2004). Role of molecular imaging in defining and denying death. J Nucl Cardiol.
9 Boersma H.H., Kietselaer B.L., Stolk L.M., Bennaghmouch A., Hofstra L., Narula J., Heidendal G.A., Reutelingsperger C.P. (2005). Past, present, and future of annexin A5: from protein discovery to clinical applications. J Nucl Med.
10 Lahorte C., Slegers G., Philippe J., Van de Wiele C., Dierckx R.A. (2001). Synthesis and in vitro evaluation of 123I-labelled human recombinant annexin V. Biomol Eng.
11 Zalutsky M.R., Narula A.S. (1987). A method for the radiohalogenation of proteins resulting in decreased thyroid uptake of radioiodine. Int J Rad Appl Instrum [A].
12 Glaser M., Collingridge D.R., Aboagye E.O., Bouchier-Hayes L., Hutchinson O.C., Martin S.J., Price P., Brady F., Luthra S.K. (2003). Iodine-124 labelled annexin-V as a potential radiotracer to study apoptosis using positron emission tomography. Appl Radiat Isot.
13 Garg P.K., Archer G.E., Bigner D.D., Zalutsky M.R. (1989). Synthesis of radioiodinated N-succinimidyl iodobenzoate: optimization for use in antibody labelling. Int J Rad Appl Instrum [A].
14 Glaser M. Collingridge E. Aboagye E. Bouchier-Hayes L. Brown D.J. Hutchinson O.C. Martin S.J. Price P. Luthra S.K. Brady F. Preparation of [124I]IBA-Annexin-V as a potential PET probe for apoptosis J. Labelled Cpd. Radiopharm 2001 44Suppl. 1S336 S338
15 Keen H.G., Dekker B.A., Disley L., Hastings D., Lyons S., Reader A.J., Ottewell P., Watson A., Zweit J. (2005). Imaging apoptosis in vivo using 124I-annexin V and PET. Nucl Med Biol.
16 Dekker B., Keen H., Shaw D., Disley L., Hastings D., Hadfield J., Reader A., Allan D., Julyan P., Watson A., Zweit J. (2005). Functional comparison of annexin V analogues labeled indirectly and directly with iodine-124. Nucl Med Biol.
17 Collingridge D.R., Glaser M., Osman S., Barthel H., Hutchinson O.C., Luthra S.K., Brady F., Bouchier-Hayes L., Martin S.J., Workman P., Price P., Aboagye E.O. (2003). In vitro selectivity, in vivo biodistribution and tumour uptake of annexin V radiolabelled with a positron emitting radioisotope. Br J Cancer.
18 Dekker B., Keen H., Zweit J., Lyons S., Smith N., Watson A., Williams G., Disley L. (2003). Detection of cell death using 124I-annexin V. J Nucl Med.